# ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-c(RGDyK)-S-S-CPLHSpT

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane-1,4,7-triacetic acid-c(RGDyK)-S-S-CPLHSpT
Abbreviated name: | ^68^Ga-NOTA-cRGDyK-CPLHSpT
Synonym:
Agent category: | Polypeptide
Target: | α_v_β_3_ integrin receptor, Polo-like kinase (PLK1)
Target category: | Receptor, enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLHSpT)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The peptide sequence Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_.

Polo-like kinase 1 (PLK1) regulates cell cycle progression during mitosis (8) and is overexpressed in many different tumors (9). The kinase activity of PLK1 is regulated by a highly conserved C-terminal polo-box domain (PBD) (10). The phosphopeptide Pro-His-Ser-p-Thr (PLHSpT) is a potent selective inhibitor of the PBD of human PLK1. However, PLHSpT does not permeate cell membranes. Binding of PLHSpT to PBD by microinjection into cancer cells induces mitotic arrest and apoptotic cell death. Kim et al. (11) designed and synthesized cRGDyK-S-S-CPLHSpT for tumor treatment and imaging of PLK1. CPLHSpT was delivered to the PLK1 in the nucleus by internalization of cRGDyK-S-S-CPLHSpT via binding of cRGDyK to the integrin receptor and cleavage of cRGDyK-S-S-CPLHSpT in the cytoplasm. For positron emission tomography (PET) imaging, ^68^Ga-1,4,7-triazacyclononane-1,4,7-triacetic acid-(cRGDyK)-S-S-CPLHSpT (^68^Ga-NOTA-cRGDyK-CPLHSpT) was evaluated in nude mice bearing human glioblastoma U87MG tumors.

### Related Resource Links:

- Chapters in MICAD (PLK1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PLK1+AND+micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (PLK1 (http://www.ncbi.nlm.nih.gov/gene/5347), α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (PLK1 (http://omim.org/entry/602098), α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (PLK1 (http://www.clinicaltrials.gov/ct2/results?term=polo-like%20kinase), RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLHSpT)]

PLHSpT and CPLHSpT were prepared using solid-phase synthesis (11). cRGDyK-S-S-CPLHSpT was prepared by conjugation of N-succinimidyl-3-(2-pyridyldithio)-propionate–activated cRGDyK and Fmoc-CPLHSpT in dimethyl formamide for 24 h at room temperature. cRGDyK-S-S-CPLHSpT was isolated with high-performance liquid chromatography (HPLC), with >99% purity. Addition of the NOTA group to cRGDyK-S-S-CPLHSpT was performed by mixing 9.7 µmol protein with 10.7 µmol SCN-Bz-NOTA in 0.1 M sodium carbonate buffer (pH 9.5) for 20 h at room temperature. NOTA-cRGDyK-S-S-CPLHSpT was purified with HPLC. For ^68^Ga labeling, a solution of 74 MBq (2 mCi) ^68^GaCl_3_ and NOTA-cRGDyK-S-S-CPLHSpT was incubated for 10 min at room temperature. ^68^Ga-NOTA-cRGDyK-S-S-CPLHSpT was purified with HPLC. The radiochemical yield was 20%–35%. The specific activity and radiochemical purity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLHSpT%20and%20in%20vitro)]

Cellular accumulation of 30 µM FITC-cRGDyK-S-S-CPLHSpT and FITC-PLHSpT was studied in human glioblastoma U87MG cells (positive for α_v_β_3_ integrin and PLK1) and human cervical cancer HeLa cells (positive for α_v_β_3_ integrin and PLK1) for 3 h in culture (11). Fluorescence imaging analysis showed localization of fluorescence signal from FITC-cRGDyK-S-S-CPLHSpT in the nuclei and surroundings, whereas little fluorescence signal was observed with FITC-PLHSpT. Internalization of PLHSpT was increased by conjugation with the cRGDyK peptide.

In vitro cell viability of U87MG and HeLa cells was assessed after incubation with various concentrations (10, 50, 100, and 200 µM) of cRGDyK, PLHSpT, cRGDyK-Asp-CPLHSpT (control, non-cleavable), and cRGDyK-S-S-CPLHSpT for 24 h at 37°C (11). Only cRGDyK-S-S-CPLHSpT showed inhibition of cell survival, with 50% inhibition at 75 µM. cRGDyK-S-S-CPLHSpT induced morphological changes in the cells resembling apoptosis, whereas no such changes were observed with cRGDyK and PLHSpT. cRGDyK-S-S-CPLHSpT also inhibited PLK1 in the tumor cells, with 50% inhibition at ~60 µM, whereas no PLK1 inhibition was observed with cRGDyK and PLHSpT. Induction of apoptosis by cRGDyK-S-S-CPLHSpT was confirmed with annexin V binding and cleavage of poly(ADP-ribose) polymerase.

The radioactivity levels of ^68^Ga-NOTA-cRGDyK-S-S-CPLHSpT in U87MG cells were 1.49 ± 0.10%, 1.35 ± 0.22%, and 2.82 ± 0.15% incubation dose at 30, 60, and 120 min of incubation, respectively (11). Similar accumulation levels were observed in HeLa cells. Incubation with excess cRGDyK (100 µg/ml) inhibited the radioactivity in these cells by ~50% at 120 min of incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLHSpT%20and%20rodentia)]

Kim et al. (11) performed ex vivo biodistribution studies of 3.7 MBq (0.1 mCi) ^68^Ga-NOTA-cRGDyK-S-S-CPLHSpT in nude mice (n = 3/group) bearing U87MG xenografts at 30, 60, and 120 min after injection. The tumor accumulation of radioactivity was 1.02 ± 0.25% injected dose/gram (ID/g), 3.40 ± 1.10% ID/g, and 0.62 ± 0.05% ID/g at 30, 60, and 120 min, respectively. The organ with the highest accumulation at 60 min was the liver (18% ID/g), followed by the kidney (16% ID/g), spleen (7% ID/g), lung (4% ID/g), femur (3% ID/g), heart (2% ID/g), muscle (2% ID/g), and brain (<1% ID/g). The blood concentration at 60 min was 5% ID/g. No blocking studies were performed.

Kim et al. (11) performed whole-body PET imaging in nude mice (n = 3) bearing U87MG tumors at 30, 60, and 120 min after intravenous injection of 7.2 MBq (0.2 mCi) ^68^Ga-NOTA-cRGDyK-S-S-CPLHSpT. The tumor was clearly visualized at 30 min and 60 min, whereas the liver and kidneys had the highest radioactivity levels and were clearly visualized at 30, 60, and 120 min. Region-of-interest analysis in the tumors showed standardized uptake values of 1.22 ± 0.11, 1.45 ± 0.10, and 0.85 ± 0.05 at 30, 60, and 120 min, respectively. The tumor/background ratios at 30, 60, and 120 min were 2.55, 3.03, and 1.81, respectively. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLHSpT%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLHSpT%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PLHSpT%20and%20human)]

No publication is currently available.

## References

1 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
2 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
3 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
4 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
5 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
6 Varner J.A., Cheresh D.A. (1996). Integrins and cancer. Curr Opin Cell Biol.
7 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
8 Barr F.A., Sillje H.H., Nigg E.A. (2004). Polo-like kinases and the orchestration of cell division. Nat Rev Mol Cell Biol.
9 Takai N., Hamanaka R., Yoshimatsu J., Miyakawa I. (2005). Polo-like kinases (Plks) and cancer. Oncogene.
10 Yun S.M., Moulaei T., Lim D., Bang J.K., Park J.E., Shenoy S.R., Liu F., Kang Y.H., Liao C., Soung N.K., Lee S., Yoon D.Y., Lim Y., Lee D.H., Otaka A., Appella E., McMahon J.B., Nicklaus M.C., Burke T.R., Yaffe M.B., Wlodawer A., Lee K.S. (2009). Structural and functional analyses of minimal phosphopeptides targeting the polo-box domain of polo-like kinase 1. Nat Struct Mol Biol.
11 Kim S.M., Yoon S., Choi N., Hong K.S., Murugan R.N., Cho G., Ryu E.K. (2012). In vivo tumor imaging using polo-box domain of polo-like kinase 1 targeted peptide. Biomaterials.